# ^111^In-Diethylenetriaminepentaacetic acid-cyclo(CTTHWGFTLC)

Chemical name: | ^111^In-Diethylenetriaminepentaacetic acid- cyclo(CTTHWGFTLC)
Abbreviated name: | ^111^In-DTPA-CTT
Synonym:
Agent category: | Peptide
Target: | Gelatinases (MMP-2 and MMP-9)
Target category: | Enzyme
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DTPA-CTT)]

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans surrounding connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Invasive tumor cells adhere to the ECM components, which provide a matrix environment for their permeation through the basal lamina and underlying interstitial stroma of the connective tissue by matrix metalloproteinases (MMPs), which degrade the basement membrane and ECM (3).

Gelatinase family is a subgroup of MMPs consisting of gelatinase A (MMP-2) and B (MMP-9) (4). Gelatinase expression in normal cells, such as trophoblasts, osteoclasts, neutrophils and macrophages, is highly regulated. Elevated level of gelatinases has been found in tumors associated with a poor prognosis in cancer patients (5). A cyclic decapeptide, cCTTHWGFTLC (CTT), was found to be a potent and selective inhibitor of MMP-2 and MMP-9 (6). The HWGF motif is important for the inhibitory activity. Diethylenetriaminepentaacetic acid was conjugated to an amino group of the N-terminal cysteine of the CTT peptide for radiolabeling with ^111^In. ^111^In-DTPA-CTT is being developed for single-photon emission computed tomography (SPECT) imaging of gelatinase activity in metastatic tumors.

### Related Resource Links:

- Chapters in MICAD (MMP (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=matrix+metalloproteinases+AND+micad%5Bbook%5D))
- Gene information in NCBI (MMP2 (http://www.ncbi.nlm.nih.gov/gene/4313), MMP9 (http://www.ncbi.nlm.nih.gov/gene/4318))
- Articles in Online Mendelian Inheritance in Man (OMIM) (MMP2 (http://omim.org/entry/120360), MMP9 (http://omim.org/entry/120361))
- Clinical trials (MMP (http://www.clinicaltrials.gov/ct2/results?term=matrix+metalloproteinases))
- Drug information in FDA (MMP (http://google2.fda.gov/search?q=matrix+metalloproteinases+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=10&y=10))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DTPA-CTT%20synthesis)]

A mixture of 3.7-7.4 MBq (0.1-0.2 mCi) ^111^InCl_3_ and DTPA-CTT (10 μg) was incubated in 0.1 M acetic acid for 30 min at room temperature (7). ^111^In-DTPA-CTT was purified by high-performance liquid chromatography to have a radiochemical purity of >95%. The specific activity was >400 MBq/µmol (10.8 mCi/µmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DTPA-CTT%20synthesis%20and%20in%20vitro)]

Hanaoka et al. (7) reported that In-DTPA-CTT inhibited the proteolytic activity of MMP-2 with an IC_50_ value of 1026 μM, whereas CTT had an IC_50_ value of 283 μM. ^111^In-DTPA-CTT was ~85% intact in murine serum for 3 h at 37°C.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DTPA-CTT%20and%20rodentia)]

Hanaoka et al. (7) performed biodistribution studies in nude mice (n = 4-5) bearing human breast carcinoma MDA-MB-231 (high gelatinase expression) or MDA-MB-435S (low gelatinase expression) xenografts. ^111^In-DTPA-CTT cleared rapidly from the blood with 0.09 ± 0.01% injected dose (ID)/g for the MDA-MB-231 and 0.16 ± 0.04% ID/g for the MDA-MB-435S tumors at 3 h. The tumor/blood ratio was 2.81 and 0.94 at 3 h, respectively. Accumulation of radioactivity was low in the liver (0.12-0.23% ID/g) and muscle (<0.01% ID/g). The majority of the radioactivity was excreted via the kidneys (7.8-9.19% ID/g at 3 h) into urine. There is a significant correlation (r = 0.801) between tumor accumulation and gelatinase activity. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DTPA-CTT%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DTPA-CTT%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DTPA-CTT%20and%20human)]

No publication is currently available.

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
4 Nelson A.R., Fingleton B., Rothenberg M.L., Matrisian L.M. (2000). Matrix metalloproteinases: biologic activity and clinical implications. J Clin Oncol.
5 Deryugina E.I., Quigley J.P. (2006). Matrix metalloproteinases and tumor metastasis. Cancer Metastasis Rev.
6 Koivunen E., Arap W., Valtanen H., Rainisalo A., Medina O.P., Heikkila P., Kantor C., Gahmberg C.G., Salo T., Konttinen Y.T., Sorsa T., Ruoslahti E., Pasqualini R. (1999). Tumor targeting with a selective gelatinase inhibitor. Nat Biotechnol.
7 Hanaoka H., Mukai T., Habashita S., Asano D., Ogawa K., Kuroda Y., Akizawa H., Iida Y., Endo K., Saga T., Saji H. (2007). Chemical design of a radiolabeled gelatinase inhibitor peptide for the imaging of gelatinase activity in tumors. Nucl Med Biol.